# N-[^18^F]Fluoroacetyl-N-(2,5-dimethoxybenzyl)-2-phenoxyaniline

Chemical name: | N-[^18^F]Fluoroacetyl-N-(2,5-dimethoxybenzyl)-2-phenoxyaniline
Abbreviated name: | [^18^F]PBR06
Synonym:
Agent category: | Compound
Target: | Peripheral-type benzodiazepine receptor (PBR), also known as translocator protein (TSPO)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR06%5BAll%20Fields%5D)]

Benzodiazepines are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been designated as central benzodiazepine receptors (CBR) and peripheral benzodiazepine receptors (PBR). PBR is also known as translocator protein (TSPO). The CBR is found exclusively in the central nervous system on the membranes of neurons and is coupled to the γ-aminobutyric acid receptor/chloride channel (3). In contrast, the PBR is a mitochondrial protein found in brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4). The brain has lower levels of PBR than do the peripheral tissues. Both glial cells and macrophages contain high levels of PBR (5-7). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage that accompanies several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBRs have been studied in vivo by positron emission tomography (PET) using 1-(2-chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide ([^11^C]PK11195), an isoquinoline carboxamide with specific PBR antagonistic activity (8). [^11^C]PK11195 has been developed as a PET agent for non-invasive studies of microglia and macrophage activation in the brain, lung, and heart. However, accumulation of this tracer in the brain is limited. N-(2,5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide (DAA1106) was found to be a selective agonist for studying PBRs in the central nervous system (9, 10). DAA1106 was reported to have a higher affinity for PBRs in mitochondrial fractions of rat and monkey brains than PK11195 (9, 10). Therefore, both tracers are able to cross the normal cell membrane to reach the mitochondrial receptor sites. N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^18^F]fluoroethyl-5-methoxybenzyl)acetamide ([^18^F]FEDAA1106) and [^11^C]DAA1106 have been developed as potential PET ligands with highly selective and specific binding to PBR (11, 12). N-[^18^F]Fluoroacetyl-N-(2,5-dimethoxybenzyl)-2-phenoxyaniline ([^18^F]PBR06), which has an aryloxyanilide structure, has been evaluated for imaging PBR in the brain.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PBR%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=706%5Buid%5D))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=109610)
- Clinical trials (PBR (http://www.clinicaltrials.gov/ct2/results?term=pk11195+OR+PBR))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR06%20and%20synthesis)]

Imaizumi et al. (13) reported the synthesis of [^18^F]PBR06 by nucleophilic displacement of the bromo precursor with [^18^F]KF/Kryptofix 2.2.2./K_2_CO_3_ at 110°C for 10 min and purified by high-performance liquid chromatography. The specific activity was 26.8 ± 17.5 GBq/μmol (0.72 ± 0.47 Ci/μmol) at the time of injection with 10–20% radiochemical yield.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR06%20and%20in%20vitro)]

In vitro [^3^H]PK11195 PBR-binding studies using monkey brain mitochondrial homogenates showed inhibition constant (K_i_) values of 0.30 ± 0.08nM and 3.84 ± 1.26 nM for PBR06 and PK11195, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR06%20and%20rodentia)]

No publications are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR06%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR06%20and%20%28primate%20not%20human%29)]

Imaizumi et al. (13) reported PET studies of [^18^F]PBR06 in the monkey brain. The radioactivity level of [^18^F]PBR06 in the monkey brain was 300% of the standard uptake value with greater radioactivity in gray matter than in white matter. [^18^F]PBR06 exhibited the highest uptake in the choroid plexus, a region rich in PBR. Accumulation of [^18^F]PBR06 in the cerebellum, putamen, and choroid plexus was inhibited significantly (~80%) by pretreatment of DAA1106 (3 mg/kg), indicating that the binding of [^18^F]PBR06 in the monkey brain was mainly attributable to PBR. Averaged distribution volume (V_T_) values by a two-tissue compartment model were 60, 80, and 78 ml/cm^3^ in the cerebellum, putamen, and choroid plexus, respectively. V_T_ values by a one-tissue compartment model were 49, 65, and 49 ml/cm^3^ in the cerebellum, putamen, and choroid plexus, respectively. In the blocking experiment, V_T_ values by a one-tissue compartment model were 2.0, 2.4, and 2.3 ml/cm^3^ in the cerebellum, putamen, and choroid plexus, respectively. Therefore, ~95% of V_T_ in the baseline scans was PBR-specific binding. The V_T_ value was more stable and more reliably determined with 200 min of baseline scanning using the two-compartment model than the one-compartment model. Approximately 20–30% of radioactivity in the plasma was intact [^18^F]PBR06 at 5 min after injection. The metabolites were more hydrophilic than the parent compound.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR06%20and%20human)]

Fujimura et al. (14) performed PET kinetics studies of the brain for 5 h after injection of 185 MBq (5 mCi) of [^18^F]PBR06 in 9 healthy subjects. A 2-tissue compartment model was shown to be better than a 1-tissue compartment model. A brain scan of 120 min exhibited the best estimation of V_T_ value, which was stable during 60-120 min.

Fujimura et al. (15) later performed 2-dimensional dynamic scans for radiation dosimetry after injection of 185 MBq (5 mCi) of [^18^F]PBR06 in 7 healthy subjects. The highest radiation doses were in the gallbladder wall (367.0 µSv/MBq, 1380 mrem/mCi), spleen (64.5 µSv/MBq, 239 mrem/mCi), liver (46.1 µSv/MBq, 170 mrem/mCi), kidneys (39.3 µSv/MBq, 146 mrem/mCi), lung (36.5 µSv/MBq, 135 mrem/mCi), and urinary bladder wall (31.0 µSv/MBq, 115 mrem/mCi). The effective dose was 18.5 µSv/MBq (69 mrem/mCi).

## NIH Support

Intramural research program

## References

1 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
2 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
6 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
7 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
8 Gerhard A., Neumaier B., Elitok E., Glatting G., Ries V., Tomczak R., Ludolph A.C., Reske S.N. (2000). In vivo imaging of activated microglia using [11C]PK11195 and positron emission tomography in patients after ischemic stroke. Neuroreport.
9 Okuyama S., Chaki S., Yoshikawa R., Ogawa S., Suzuki Y., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Neuropharmacological profile of peripheral benzodiazepine receptor agonists, DAA1097 and DAA1106. Life Sci.
10 Chaki S., Funakoshi T., Yoshikawa R., Okuyama S., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Binding characteristics of [3H]DAA1106, a novel and selective ligand for peripheral benzodiazepine receptors. Eur J Pharmacol.
11 Fujimura Y., Ikoma Y., Yasuno F., Suhara T., Ota M., Matsumoto R., Nozaki S., Takano A., Kosaka J., Zhang M.R., Nakao R., Suzuki K., Kato N., Ito H. (2006). Quantitative analyses of 18F-FEDAA1106 binding to peripheral benzodiazepine receptors in living human brain. J Nucl Med.
12 Maeda J., Suhara T., Zhang M.R., Okauchi T., Yasuno F., Ikoma Y., Inaji M., Nagai Y., Takano A., Obayashi S., Suzuki K. (2004). Novel peripheral benzodiazepine receptor ligand [11C]DAA1106 for PET: an imaging tool for glial cells in the brain. Synapse.
13 Imaizumi M., Briard E., Zoghbi S.S., Gourley J.P., Hong J., Musachio J.L., Gladding R., Pike V.W., Innis R.B., Fujita M. (2007). Kinetic evaluation in nonhuman primates of two new PET ligands for peripheral benzodiazepine receptors in brain. Synapse.
14 Fujimura Y., Zoghbi S.S., Simeon F.G., Taku A., Pike V.W., Innis R.B., Fujita M. (2009). Quantification of translocator protein (18 kDa) in the human brain with PET and a novel radioligand, (18)F-PBR06. J Nucl Med.
15 Fujimura Y., Kimura Y., Simeon F.G., Dickstein L.P., Pike V.W., Innis R.B., Fujita M. (2010). Biodistribution and radiation dosimetry in humans of a new PET ligand, (18)F-PBR06, to image translocator protein (18 kDa). J Nucl Med.